# N1’-([^11^C]Methyl)naltrindole

Chemical name: | N1’-([^11^C]Methyl)naltrindole
Abbreviated name: | [^11^C]MeNTI
Synonym:
Agent category: | Compound
Target: | Delta (δ) opioid receptor
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%5BAll%20Fields%5D%20AND%20MeNTI%5BAll%20Fields%5D)]

Opioids such as morphine are commonly used analgesics in clinical practice. Three opioid receptors (mu, µ; delta, δ; and kappa, κ) that mediate opioid effects have been identified by molecular cloning: δ (enkephalin-preferring), κ (dynorphin-preferring), and µ (morphine and ß-endorphin-preferring) (1). Each type of opioid receptors consists of subtypes of receptors as suggested by pharmacological studies (2, 3). Their specificity and ubiquitous location are present in both the central and peripheral nervous system. The opioid receptors (G-protein coupled, resulting in decrease in adenylyl cyclase activity) play an important role in the regulation of analgesia, shock, appetite, thermoregulation, cardiovascular, mental and endocrine function (2-5). Although µ opioid receptors are the major receptor to mediate the analgesic effects of opioids, δ and κ receptors are also important in antinociception. Opioids have been found to protect cells from ischemia injury in the heart and brain via the δ receptors. On the other hand, κ antagonist prevents neurodegeneration.

The µ opioid receptors are localized predominately in the hypothalamus and thalamus, and the δ opioid receptors are localized predominately in the striatum, limbic system, and cerebral cortex (6, 7). The κ opioid receptors (κ_1_ and κ_2_ ) are the most abundant brain opioid receptors and are widely distributed in deeper layers of the neocortex (particularly temporal, parietal, and frontal cortices), striatum, amygdala, and thalamus, with lower levels in the hippocampus, occipital cortex, and cerebellum (8-10). The µ opioid receptors have been implicated in several clinical brain disorders, including drug and alcohol abuses, epilepsy, and pain pathways.

Carfentanil (CFN) is a highly potent and selective µ opioid receptor agonist with subnanomolar affinity (K_d_, 0.08 nM). [^11^C]CFN (http://www.ncbi.nlm.nih.gov/books/NBK23273/) is being developed as a positron emission tomography (PET) agent for the non-invasive studies of µ opioid receptors in the brain. On the other hand, N1’-methylnaltrindole (MeNTI) is a potent and selective δ opioid receptor antagonist (K_i_, 0.02 nM). [^11^C]MeNTI has been prepared for studying the role of δ opioid receptor in health and disease by PET imaging.

### Related Resource Links:

- Chapters in MICAD (opioid receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=opioid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (µ opioid receptor (http://www.ncbi.nlm.nih.gov/gene/4988), δ opioid receptor (http://www.ncbi.nlm.nih.gov/gene/4985))
- Articles in Online Mendelian Inheritance in Man (OMIM) (µ opioid receptor (http://www.ncbi.nlm.nih.gov/omim/600018), δ opioid receptor (http://www.ncbi.nlm.nih.gov/omim/165195))
- Clinical trials (opioid receptors (http://www.clinicaltrials.gov/ct2/results?term=opioid+receptors+))
- Drug information in FDA (opioid receptors (http://google2.fda.gov/search?q=opioid+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20MeNTI%20and%20synthesis)]

Lever et al. (11) reported synthesis of [^11^C]MeNTI by [^11^C]-N-methylation of 3-O-benzylnaltrindole with [^11^C]iodomethane, and final hydrogenolysis of the benzyl protecting group. An average radiochemical yield was 6% (based on [^11^C]iodomethane) with a total synthesis time of 24 min from end of bombardment. An average specific activity was 76 GBq/μmol (2.05 Ci/μmol) at end of synthesis with a radiochemical purity of >99%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20MeNTI%20and%20in%20vitro)]

Portoghese et al. (12) reported that MeNTI had K_i_ values of 0.02, 14, and 65 nM for the δ, µ, and κ opioid receptors, respectively. Therefore, MeNTI exhibits excellent overall selectivity of 700-fold δ over µ receptors and >3200-fold δ over κ receptors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20MeNTI%20and%20rodentia)]

Biodistribution studies in mice injected with 14.5 MBq (0.4 mCi) [^11^C]MeNTI were performed by Lever et al. (11) showing high accumulation of radioactivity in the striatum, olfactory tubercles and cortex, followed by hippocampus, thalamus, hypothalamus and cerebellum at 15-90 min post injection. The regional accumulation correlated linearly with in vitro receptor binding in similar brain regions (r = 0.93). Pretreatment with naltrindole (a δ opioid receptor antagonist) decreased accumulation of radioactivity in the striatum, olfactory tubercles and cortex by 65-75% but not by cyprodime (a µ antagonist) and U50,488 (a κ agonist).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20MeNTI%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20MeNTI%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20MeNTI%20and%20human)]

Madar et al. (13) reported PET studies in normal human brain (n = 4) using [^11^C]MeNTI. [^11^C]MeNTI accumulation was highest in regions of the neocortex (insular, parietal, frontal, cingulate, and occipital), caudate nucleus, and putamen. Binding was intermediate in the amygdala and lowest in the cerebellum and thalamus. Naltrexone pretreatment inhibited [^11^C]MeNTI binding effectively in δ receptor-rich regions, and its inhibitory potency correlated well (r = 0.88) with the in vitro regional distribution of δ opioid sites from postmortem human brains.

Madar et al. (14) performed PET studies in patients (n = 10) with temporal lobe epilepsy. Paired measurements of δ and µ opioid receptor binding and metabolic activity were performed with PET using [^11^C]MeNTI and [^11^C]CFN and [^18^F]fluorodeoxyglucose ([^18^F]FDG (http://www.ncbi.nlm.nih.gov/books/NBK23335/)), respectively. Binding of [^11^C]MeNTI and [^11^C]CFN increased and [^18^F]FDG uptake decreased in the temporal cortex (TC) ipsilateral to the epileptic focus. Decreases in [^18^F]FDG uptake were more widespread regionally than were increases in opioid receptors. Increases in µ receptor binding were confined to the middle region of the inferior TC, whereas binding of δ receptors increased in the mid-inferior TC and anterior region of the middle and superior TC.

Madar et al. (15) performed PET studies in patients (n = 7) with lung carcinoma. Elevated tumor binding of [^11^C]MeNTI and [^11^C]CFN was detected in all but one patient with a large necrotic center in the tumor. The mean [^11^C]MeNTI tumor's standard uptake value (SUV) was 7.4 ± 0.85 compared with 1.8 ± 0.44 in the healthy lung tissue. [^11^C]CFN binding in tumor was significantly (P = 0.003) lower than that of [^11^C]MeNTI. The average [^11^C]CFN SUVs in tumor and host lung were 2.7 ± 0.72 and 0.91 ± 0.25, respectively. The mean specific/nonspecific binding ratio was greater for [^11^C]MeNTI (4.32 ± 1.30) than that for [^11^C]CFN (2.42 ± 1.17). Naloxone treatment inhibited 50% and 44% of the specific/nonspecific binding ratios of [^11^C]MeNTI and [^11^C]CFN, respectively. The mean [^18^F]FDG SUVs in tumor and host lung (n = 4) were 5.70 ± 1.29 and 0.66 ± 0.14, respectively.

## References

1 Minami M., Satoh M. (1995). Molecular biology of the opioid receptors: structures, functions and distributions. Neurosci Res.
2 Waldhoer M., Bartlett S.E., Whistler J.L. (2004). Opioid receptors. Annu Rev Biochem.
3 Satoh M., Minami M. (1995). Molecular pharmacology of the opioid receptors. Pharmacol Ther.
4 Molina P.E. (2006). Opioids and opiates: analgesia with cardiovascular, haemodynamic and immune implications in critical illness. J Intern Med.
5 Barry U., Zuo Z. (2005). Opioids: old drugs for potential new applications. Curr Pharm Des.
6 Chang K.J., Cooper B.R., Hazum E., Cuatrecasas P. (1979). Multiple opiate receptors: different regional distribution in the brain and differential binding of opiates and opioid peptides. Mol Pharmacol.
7 Pfeiffer A., Pasi A., Mehraein P., Herz A. (1982). Opiate receptor binding sites in human brain. Brain Res.
8 Peckys D., Landwehrmeyer G.B. (1999). Expression of mu, kappa, and delta opioid receptor messenger RNA in the human CNS: a 33P in situ hybridization study. Neuroscience.
9 Hiller J.M., Fan L.Q. (1996). Laminar distribution of the multiple opioid receptors in the human cerebral cortex. Neurochem Res.
10 Simonin F., Gaveriaux-Ruff C., Befort K., Matthes H., Lannes B., Micheletti G., Mattei M.G., Charron G., Bloch B., Kieffer B. (1995). kappa-Opioid receptor in humans: cDNA and genomic cloning, chromosomal assignment, functional expression, pharmacology, and expression pattern in the central nervous system. Proc Natl Acad Sci U S A.
11 Lever J.R., Scheffel U., Kinter C.M., Ravert H.T., Dannals R.F., Wagner H.N., Frost J.J. (1992). In vivo binding of N1'-([11C]methyl)naltrindole to delta-opioid receptors in mouse brain. Eur J Pharmacol.
12 Portoghese P.S., Sultana M., Takemori A.E. (1990). Design of peptidomimetic delta opioid receptor antagonists using the message-address concept. J Med Chem.
13 Madar I., Lever J.R., Kinter C.M., Scheffel U., Ravert H.T., Musachio J.L., Mathews W.B., Dannals R.F., Frost J.J. (1996). Imaging of delta opioid receptors in human brain by N1'-([11C]methyl)naltrindole and PET. Synapse.
14 Madar I., Lesser R.P., Krauss G., Zubieta J.K., Lever J.R., Kinter C.M., Ravert H.T., Musachio J.L., Mathews W.B., Dannals R.F., Frost J.J. (1997). Imaging of delta- and mu-opioid receptors in temporal lobe epilepsy by positron emission tomography. Ann Neurol.
15 Madar I., Bencherif B., Lever J., Heitmiller R.F., Yang S.C., Brock M., Brahmer J., Ravert H., Dannals R., Frost J.J. (2007). Imaging delta- and mu-opioid receptors by PET in lung carcinoma patients. J Nucl Med.